# ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-isothiocyanatobenzyl-c(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-isothiocyanatobenzyl-c(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | ^68^Ga-NOTA-RGD, ^68^Ga-NOTA-SCN-Bz-c(RGDyK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (IC_50_, 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Jeong et al. (13) used 2-(p-isothiocyanatobenzyl)-1,4,7-triazacyclononane-1,4-7-triacetic acid (SCN-Bz-NOTA) as a bifunctional chelator for labeling c(RGDyK) to form ^68^Ga-1,4,7-triazacyclononane-1,4-7-triacetic acid-isothiocyanatobenzyl-c(Arg-Gly-Asp-D-Tyr-Lys) (^68^Ga-NOTA-RGD) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+synthesis)]

Addition of a NOTA group to RGD was performed by mixing 0.60 µmol RGD with 0.66 umol SCN-Bz-NOTA in sodium carbonate buffer (pH 9.5) for 20 h at room temperature (13). SCN-Bz-NOTA-RGD was isolated with high-performance liquid chromatography (HPLC). MALDI-TOF-MS was m/z 1,071 (calculated molecular weight, 1,069.5). For ^68^Ga labeling, a solution of 740 MBq (20 mCi) ^68^GaCl_3_ and 30 nmol RGD was heated for 10 min at room temperature. ^68^Ga-NOTA-RGD was purified with HPLC, with a yield of 89% and a radiochemical purity of >98%. The specific activity was 17.4 GBq/µmol (0.47 Ci/µmol) at the end of purification. ^68^Ga-NOTA-RGD was stable for >4 h at room temperature.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+in+vitro)]

Jeong et al. (13) performed in vitro inhibition studies of NOTA-RGDand human α_v_β_3_ integrin with ^125^I-c(RGDyK). The inhibition constant values were 1.3 nM and 1.9 nM for c(RGDyK) and NOTA-RGD, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+%20rodentia)]

Jeong et al. (13) performed ex vivo biodistribution studies of 5.6 MBq (0.15 mCi) ^68^Ga-NOTA-RGD in nude micebearing human colon cancer SNU-C4 xenografts at 1 h and 2 h after injection. Tumor and kidney accumulation values were 5.1 ± 1.0% and 5.3 ± 1.3% injected dose per gram (ID/g) at 1 h after injection, respectively. Lower levels were observed in the liver, intestines, lung, spleen, and heart (<2.2% ID/g). The tumor/blood and tumor/muscle ratios at 1 h after injection were 10.3 ± 4.8 and 9.3 ± 3.9, respectively. PET imaging in the tumor-bearing micewas performed with 16 MBq (0.43 mCi) ^68^Ga-NOTA-RGD at 1 h and 2 h after injection. The tumors were clearly visualized at these two time points. High levels of radioactivity were found in the kidneys and urinary bladder, with less accumulation in the liver and intestine. Co-injection of excess c(RGDyK) reduced the tumor accumulation to the background level at 1 h after injection. The radioactivity levels in the liver and kidneys were also reduced. In another experiment, ^68^Ga-NOTA-RGD accumulation in ischemic hind limb muscle (1.6 ± 0.2% ID/g) was reduced significantly with c(RGDyK) to near the level in normal hind limb (0.5 ± 0.1% ID/g, P < 0.01).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Jeong J.M., Hong M.K., Chang Y.S., Lee Y.S., Kim Y.J., Cheon G.J., Lee D.S., Chung J.K., Lee M.C. (2008). Preparation of a promising angiogenesis PET imaging agent: 68Ga-labeled c(RGDyK)-isothiocyanatobenzyl-1,4,7-triazacyclononane-1,4,7-triacetic acid and feasibility studies in mice. J Nucl Med.